# Radioiodinated-anti–TAG-72 covalently linked CC49 divalent single-chain Fv antibody

Chemical name: | Radioiodinated-anti–TAG-72 covalently linked CC49 divalent single-chain Fv antibody
Abbreviated name: | ^125^I-CC49 sc(Fv)_2_ Ab
Synonym: | ^125^I-CC49 Ab, ^125^I-CC49 divalent single-chain Fv recombinant antibody, ^125^I-CC49 covalent sc(Fv)_2_ Ab
Agent Category: | Divalently linked CC49 divalent single-chain Fv antibody construct sc(Fv)_2_ Ab
Target: | (Sialyl-Tn (STn)) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission tomography (SPECT), planar gamma imaging
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))]

Radioiodinated-anti–TAG-72 covalently linked CC49 divalent single-chain Fv antibody (^125^I-CC49 sc(Fv)_2_ Ab), which is formed by the conjugation of ^125^I with a bioengineered recombinant anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for gamma imaging of cancers that express TAG-72 (1). ^125^I has a physical half-life (t_½_) of 60 days with a gamma energy that is not ideal for in vivo imaging, but there are other radioactive iodines (^123^I, ^131^I) available that are more suitable for single-photon emission tomography (SPECT) and planar gamma imaging.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (2-5). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (6). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 mucin was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (7). With the use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-72 MAbs with higher affinity constants (K_a_) have been produced and characterized (2, 3, 7, 8). CC49 MAb appears to react with a unique disaccharide sialyl-Tn (STn) epitope on the TAG-72 (1, 9).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (10). Radiolabeled B72.3 and CC49 have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (11, 12). Because of their relatively large size, radiolabeled intact MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (8, 13-15). One approach to minimize these problems is reducing intact antibodies to antibody fragments such as F(ab’)_2_ and Fab’ (16). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (8, 17, 18). These scFv constructs contain the variable regions of the light chain (V_L_) and heavy chain (V_H_) connected by a flexible linker. Colcher et al. (19) constructed the monomeric CC49 scFv Ab (~27 kDa), which selectively recognizes a unique STn epitope of TAG-72. The radioiodinated CC49 scFv appeared to clear rapidly from the blood with good tumor penetration (18, 20). To further improve the imaging kinetics by use of multivalency as a means of increasing the functional affinity, Beresford et al. (1) reported the construction of a high-affinity covalently linked dimer CC49 sc(Fv)_2_ (~58 kDa). This dimeric structure does not rely on non-covalent interactions and is designated as sc(Fv)_2_ to distinguish it from the non-covalently linked dimer (scFv)_2_ derived from the monomeric construct. CC49 sc(Fv)_2_ does not require additional chemical processing for in vivo studies. The radioiodinated CC49 sc(Fv)_2_ showed good stability and improved in vivo pharmacokinetics compared with the radioiodinated non-covalently linked CC49 (scFv)_2_ construct and intact CC49 IgG.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+synthesis)]

Beresford et al. (1) reported the construction and radiolabeling of the ^125^I-CC49 sc(Fv)_2_ Ab. The covalent CC49 scFv (V_L_-linker-V_H_) was derived from the murine MAb CC49 and constructed with the 205C linker with 25 amino acids (LSADDAKKDAAKKDDAKKDDAKKDL) (21). The dimer sc(Fv)_2_ (V_L_-linker-V_H_-linker-V_L_-linker-V_H_) was constructed by covalently linking the two repeating chains of V_L_ and V_H_ in tandem with use of the same helical linker between each region. The nucleotide sequence of the sc(Fv)_2_ construct was cloned into the pRW83 vector (1). The expression plasmid was transformed into Escherichia coli strain AG1 or BL21. The CC49 sc(Fv)_2_ protein was prepared from the peri-plasmic fraction of 16- to 18-hr cultures. After separation, sc(Fv)_2_ was purified by ion-exchange and size-exclusion chromatography. The preparation was shown to be >90% pure by sodium dodecylsulfate–polyacrylamide gel electrophoresis (SDS-PAGE), and the protein migrated to its theoretical molecular weight.

Radioiodination of CC49 sc(Fv)_2_ Ab was performed with the use of 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) as the oxidizing agent (1). Briefly, 20–100 μg of CC49 sc(Fv)_2_ Ab in 0.1 M sodium phosphate buffer (pH 7.2) was added to a glass tube coated with 20 μg IodoGen. Approximately 0.014-0.027 MBq (0.5–1.0 mCi) ^125^I-labeled sodium iodide was added and the mixture was incubated for 3 min. Size-exclusion chromatography was performed immediately to purify the radiolabeled antibody. The labeling efficiency was 50%. The specific activity of ^125^I-CC49 sc(Fv)_2_ Ab was ~111–333 MBq/mg (3–9 mCi/mg) or 6.44–19.3 MBq/nmol (0.17–0.522 mCi/nmol) on the basis of the molecular mass of 58 kDa. The SDS-PAGE analysis showed a radiochemical purity of ~90%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))AND+in+vitro)]

The immunoreactivity of radioiodinated CC49 sc(Fv)_2_ Ab was assessed by the solid-phase radioimmunoassay (RIA), with bovine submaxillary gland mucin (BSM) as the protein antigen attached to a solid-phase matrix (1). The specific binding for radioiodinated CC49 sc(Fv)_2_ Ab was 94%, and the nonspecific binding was 2%. In a competitive RIA, the ^125^I-CC49 sc(Fv)_2_ Ab was completely inhibited by CC49 IgG, F(ab’)2 and Fab’ for binding to BSM (1). The binding kinetics of ^125^I-CC49 sc(Fv)_2_ Ab was assessed by the real-time kinetic analysis with use of a surface plasmon resonance detector (1). The study reported the association constant (K_a_) of unlabeled CC49 sc(Fv)_2_ to be 3.34 × 10^7^ M−^1^. In comparison, the K_a_ for the intact CC49 MAb and the non-covalently linked CC49 (scFv)_2_ construct were 1.14 × 10^8^ M−^1^ and 4.46 × 10^7^ M−^1^, respectively.

In vitro stability studies of ^125^I-CC49 sc(Fv)_2_ Ab showed that it was stable for at least 14 days when stored at 4ºC. No significant protein degradation or radioactive iodine release was observed. Only a 5−10% loss in immunoreactivity was observed over a 2-week period. Unlabeled sc(Fv)_2_ was stable at −70ºC for 5 months without loss of immunoreactivity. When ^125^I/^131^I-CC49 sc(Fv)_2_ Ab was incubated in murine serum or 1% BSA and incubated at 37ºC for up to 48 h, high-performance liquid chromatography analysis of 24−48 hr samples showed only a small increase in high molecular weight forms.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+rodentia)]

Biodistribution studies of ^125^I-CC49 sc(Fv)_2_ Ab were performed in nude mice bearing s.c. LS-174T human colon carcinomas (1). Dual-label biodistribution studies were conducted with simultaneous i.v. administration of 0.185 MBq (5 μCi) ^125^I-CC49 sc(Fv)_2_ Ab and 0.0925 MBq (2.5 μCi) ^131^I-non-covalently linked CC49 (scFv)_2_Ab and euthanized at various time points in groups of mice (n = 5−6). The average tumor radioactivity levels of ^125^I-CC49 sc(Fv)_2_Ab in percent injected dose per gram (% ID/g) were 6.12 (0.5 h), 6.63 (1 h), 6.78 (4 h), 6.27 (6 h), 5.74 (9 h), 4.67 (16 h), 4.29 (24 h), 2.62 (48 h), 1.94 (72 h), and 1.21 (120 h) with standard errors (SEM) <20% ID/g. There were also high radioactivity levels in the kidneys, spleen, and liver. At 0.5 h, the major organ radioactivity levels (% ID/g) were 18.30 (blood), 27.85 (kidneys), 10.01 (spleen), 5.65 (liver), 7.25 (lungs), and 4.31 (heart). By 24 h, these levels decreased to 0.07 (blood), 0.36 (kidneys), 0.18 (spleen), 0.20 (liver), 0.07 (lungs), and 0.03 (heart). The ^131^I-non-covalently linked CC49 (scFv)_2_ Ab had similar tumor localization, but there were differences in the degree of clearance from other normal tissues. As early as 0.5−1 h, the ^131^I-CC49 (scFv)_2_ Ab radioactivity levels in major organs were greater than those of ^125^I-CC49 sc(Fv)_2_Ab. This trend was maintained up to 48 h. The biggest differences were in the radioactivity levels in the liver and spleen. At 6 h, ^125^I-CC49 sc(Fv)_2_ Ab had radioactivity levels of 1.63% ID/g and 1.53% ID/g for the liver and spleen, respectively. In comparison, ^131^I-CC49 (scFv)_2_ Ab had radioactivity levels of 2.25% ID/g and 2.28% ID/g for the liver and spleen, respectively. The tumor/blood ratios of ^125^I-CC49 sc(Fv)_2_ Ab were 4.79 (6 h), 60.19 (24 h), 48.29 (48 h), 28.93 (72 h), and 27.79 (120 h). The radiolocalization indexes (ratios of % ID/g in tumor to % ID/g in normal tissue) at 24 h of ^125^I-CC49 sc(Fv)_2_ Ab were 61.3 (tumor/blood), 21.5 (tumor/liver), 23.8 (tumor/spleen), 11.9 (tumor/kidneys), and 61.3 (tumor/lungs). In comparison, the values for ^131^I-CC49 (scFv)_2_ Ab were 42.9 (tumor/blood), 14.3 (tumor/liver), 9.5 (tumor/spleen), 10.2 (tumor/kidneys), and 47.7 (tumor/lungs). The radiolocalization indexes for radiolabeled-CC49 IgG were 3.4 (tumor/blood), 6.1 (tumor/liver), 9.1 (tumor/spleen), 17.3 (tumor/kidneys), and 7.2 (tumor/lungs).

Pharmacokinetic studies of ^125^I-CC49 sc(Fv)_2_ Ab were conducted in mice bearing s.c. LS-147 tumors with a dose of 0.37 MBq (10 μCi) (1). ^125^I-CC49 sc(Fv)_2_ Ab showed rapid blood clearance with >50% cleared from the blood pool in <40 min. ^125^I-CC49 sc(Fv)_2_ Ab appeared to be eliminated by the kidneys and not retained by the extravascular space. Whole-body retention studies with a dose of 0.056 MBq (1.5 μCi) in mice bearing the tumors (n = 3) also showed rapid blood clearance.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))++AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+human)]

No publication is currently available.

## References

1 Beresford G.W., Pavlinkova G., Booth B.J., Batra S.K., Colcher D. (1999). Binding characteristics and tumor targeting of a covalently linked divalent CC49 single-chain antibody. Int J Cancer.
2 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
3 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
4 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
5 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
6 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
7 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
8 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
9 Colcher D., Pavlinkova G., Beresford G., Booth B.J., Batra S.K. (1999). Single-chain antibodies in pancreatic cancer. Ann N Y Acad Sci.
10 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
11 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
12 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
13 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
14 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
15 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
16 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55 Suppl 23 5777s 5785s 7493346
17 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
18 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
19 Colcher D., Goel A., Pavlinkova G., Beresford G., Booth B., Batra S.K. (1999). Effects of genetic engineering on the pharmacokinetics of antibodies. Q J Nucl Med.
20 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
21 Pavlinkova G., Beresford G., Booth B.J., Batra S.K., Colcher D. (1999). Charge-modified single chain antibody constructs of monoclonal antibody CC49: generation, characterization, pharmacokinetics, and biodistribution analysis. Nucl Med Biol.